# ^99m^Tc-Labeled succinimidyl-6-hydrazinonicotinate hydrochloride (SHNH)-conjugated visilizumab

Chemical name: | ^99m^Tc-Labeled succinimidyl-6-hydrazinonicotinate hydrochloride (SHNH)-conjugated visilizumab
Abbreviated name: | ^99m^Tc-SHNH-visilizumab
Synonym:
Agent Category: | Antibody
Target: | CD3 antigen
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation:
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=visilizumab)]

CD3 antigen is a protein complex that is expressed on the T cell surface and is involved in the signal transduction of T cell activation. More than 95% of the circulating T cells in blood and activated T cells in inflamed tissues express CD3 antigen (1-3). Blocking CD3 antigen with monoclonal antibodies (mAbs) has been shown to be effective in suppressing the immunoreaction in inflammatory and graft-versus-host disease conditions. OKT3 is a mouse anti-human CD3 mAb that has been widely used to prevent and treat acute allograft rejection in clinical transplantation (4-6). However, the clinical utility of OKT3 therapy is limited by inducing a neutralizing anti-mouse antibody response and a cytokine release syndrome (7, 8). The syndrome has been thought to be derived from the enormous release of cytokines, particularly TNF-α from T cells in response to the antibody, and to be attributed to the cross-linking of T cells bearing CD3 molecules and Fc receptor (FcR)-bearing immune effector cells that bind to the Fc portion of the antibodies. The cross-linking activates both the T cells and the FcR-bearing cells, leading to the massive release of cytokines (9, 10).

To reduce potential side effects and immunogenicity, Cole et al. generated a humanized version of the OKT3 mAb visilizumab (HuM291) (11). Visilizumab is characterized by decreased binding with FcRs due to the introduced mutations within the IgG_2_ Fc at amino acid residues 234 and 237 (Val to Ala), and by decreased ability to activate human complements because of the human IgG_2_ M3 isotype. Compared with OKT3 mAb, visilizumab has been shown to be much less mitogenic to T cells and to induce less toxicity from cytokine release in vivo, while retaining the ability to modulate the CD3 complex and inhibit the mixed lymphocyte reaction. The potential therapeutic effects of visilizumab have been examined in several immune system–related disorders, including ulcerative colitis, Crohn's disease, renal allograft rejection, and acute graft-versus-host disease (8, 12, 13)., However, visilizumab induces a rapid and severe lymphopenia after infusion in humans (12). The reason for this transient lymphopenia is unknown because the path of migration from blood after visilizumab infusion has not been clarified. Malviya et al. radiolabeled visilizumab with ^99m^Tc and checked its in vitro and in vivo specificity for CD3-positive cells (2). The design of this study was based on their hypothesis that the use of a radiolabeled antibody against CD3 antigen might assist in the selective detection of resting and activated T cells and thus serve as a diagnostic tool for imaging T cell traffic and lymphocytic infiltration of tissues and organs affected in autoimmune diseases. Ultimately, the use of a radiolabeled antibody would provide a rationale for treatment with anti-CD3 mAb and would serve as a tool for therapy follow-up.

### Relevant Resource Links

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CD3+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- CD3 Gene information in NCBI (http://www.ncbi.nlm.nih.gov/gene/?term=CD3+and+human)
- Clinical trials (Visilizumab (http://clinicaltrials.gov/ct2/results?term=visilizumab), OKT3 (http://clinicaltrials.gov/ct2/results?term=OKT3))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=visilizumab%20+%20imaging)]

To label visilizumab and the control antibody, Malviya et al. tested both direct and indirect labeling methods (2). The control mAb was a humanized IgG_2_ antibody without FcR and without CD3 binding. The direct labeling with ^99m^Tc was achieved with the 2-mercapthoethanol method. The indirect labeling was completed first by conjugating the heterobifunctional linker succinimidyl-6-hydrazinonicotinate hydrochloride (SHNH) with the mAb to obtain a SHNH-mAb conjugate, and then by coupling the SHNH-mAb complex with ^99m^Tc to obtain the desired product, ^99m^Tc-SHNH–mAb. With the direct method, a high labeling efficiency (~99%) with a high specific activity (≥2,600 MBq/mg (70.3 mCi/mg)) was achieved for the control mAb but not for visilizumab. The directly labeled control mAb was then used in all experiments. With the indirect method, a high labeling efficiency (≥90%) with a high specific activity (10,360–11,100 MBq/mg (280–300 mCi/mg) was obtained for visilizumab but not for the control mAb (labeling efficiency: <40%; specific activity: <4,440 MBq/mg (<120 mCi/mg)). An average of 4–10 hydrazino groups were conjugated to each molecule of visilizumab. The indirect labeling method was then used to label visilizumab, and the labeled product ^99m^Tc-SHNH–visilizumab was used in all experiments. The reason for the differences of labeling efficiency and specific activity between the two antibodies was not given. Both ^99m^Tc-SHNH–visilizumab and the ^99m^Tc-labeled control mAb were stable in human serum for up to 24 h at 37°C (87% for visilizumab and 89% for control Ab). The cysteine challenge assay also demonstrated high stability of the radiolabeled mAbs up to a 500:1 ratio between cysteine and the radiolabeled mAb. Sodium dodecyl sulphate polyacrylamide gel electrophoresis confirmed that visilizumab (in molecular weight) was not modified by the labeling procedure, as shown by a single band at 150 kDa.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=visilizumab%20+%20imaging)]

Malviya et al. first analyzed the CD3 expression on human peripheral blood mononuclear cells (hPBMCs), human lymphoma cells (HuT78), T cell–derived human acute lymphoblastic leukemia cells (CEM), and immortalized T lymphocytes (Jurkat cell line) with fluorescence-activated cell sorter analysis after staining cells with a fluorescein isothiocyanate–conjugated anti-CD3 antibody (2). The investigators observed a mean fluorescence intensity of 300 for hPBMCs (80% positive cells), 38 for CEM (50% positive cells), 18 for HuT78 (>95% positive cells), and 30 for Jurkat cells (60% positive cells), indicating different CD3 expression levels among the cell lines. hPBMCs and HuT78 were then used for experiments. Specific binding saturation on HuT78 cells was obtained at ^99m^Tc-SHNH–visilizumab concentrations of more than 5 × 10^-10^ mol, and ^99m^Tc-SHNH–visilizumab binding was displaced by a 100-fold molar excess of unlabeled antibody, indicating that ^99m^Tc-SHNH–visilizumab retained its specific binding activity with CD3 antigens expressed on HuT78 cells. The immunoreactive fraction of ^99m^Tc-SHNH–visilizumab on hPBMCs in two experiments was 68% and 75%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=visilizumab%20+%20imaging)]

To evaluate the binding ability of ^99m^Tc-SHNH–visilizumab with HuT78 cells in vivo, experiments were performed in athymic nude BALB/c nu/nu mice (n = 9) bearing subcutaneously implanted HuT78 cells in one thigh and CD3-negative tumor cells (TPC1) in the other thigh (control) (2). At 2 h after cell implantation, mice were injected in the tail vein with ^99m^Tc-SHNH–visilizumab. High-resolution γ-camera imaging showed that the uptake level in the HuT78 cells was significantly higher and visible than in CD3-negative control cells (P < 0.05). The target/background ratio increased significantly with increased numbers of HuT78 cells (0.98 ± 0.03 for 5 × 10^6^ cells, 1.17 ± 0.03 for 10 × 10^6^ cells, and 1.34 ± 0.12 for 20 × 10^6^ cells at 6 h; and 1.08 ± 0.06 for 5 × 10^6^ cells, 1.30 ± 0.17 for 10 × 10^6^ cells, and 1.56 ± 0.13 for 20 × 10^6^ cells at 24 h) (P < 0.05). A small but statistically nonsignificant increase of the cell uptake from 6 h to 24 h was observed, indicating fast binding kinetics of the ^99m^Tc-SHNH–visilizumab to target cells. In vivo competition studies with hPBMCs (2 x 10^7^ cells) showed that the uptake of ^99m^Tc-SHNH–visilizumab decreased significantly with pretreatment with an excess of unlabeled anti-CD3 mAb (96% at 6 h and 87% at 24 h). The target/background ratios in mice without and with pre-injected cold visilizumab were 1.91 ± 0.6 and 1.04 ± 0.2 at 6 h, and 3.06 ± 0.8 and 1.27 ± 0.3 at 24 h, respectively (all P < 0.05).

Biodistributions of the ^99m^Tc-labeled visilizumab and control mAb were investigated in female SCID mice reconstituted with hPBMCs (2). Immediately after intravenous reconstitution (8 × 10^6^ hPBMCs per mouse), mice were injected with visilizumab or control mAb (n = 3 mice/group) (10% injected antibodies were labeled with ^99m^Tc). With sequential imaging, ^99m^Tc-labeled visilizumab and control mAb presented different migration patterns of the lymphocytes and different biodistributions of the radioactivity. ^99m^Tc-SHNH–visilizumab, by binding to lymphocytes in blood, induced cells to accumulate in the liver (>400%) spleen (>720%), and small bowel (>230%) at levels higher than those induced by the control mAb (all P < 0.05). By contrast, ^99m^Tc-labeled control mAb showed a long resident time and high radioactivity (>140% at 3 h, P < 0.05) in the blood, with little accumulation of radioactivity in the liver and small intestine. Minor and statistically nonsignificant differences were observed in other organs, including the lung, kidney, and large bowel, with the counts being higher for ^99m^Tc-SHNH–visilizumab than for ^99m^Tc-labeled control mAb (data not shown). These results indicated that, after intravenous injection of a pharmacological dose of visilizumab, lymphocytes migrated from the blood to the liver, spleen, and small bowel. Histological examination of the organs confirmed the difference in the presence of human lymphocytes between visilizumab and control mAb–injected mice for the spleen and small bowel, but not for the liver, lungs, or large bowel. Lymph nodes and intestinal mucosa–associated lymphoid tissues showed the same behavior as the spleen in mice injected with visilizumab. These findings support the hypothesis that visilizumab induces lymphocyte migration from blood into primary and secondary lymphoid organs.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Guy C.S., Vignali D.A. (2009). Organization of proximal signal initiation at the TCR:CD3 complex. Immunol Rev.
2 Malviya G., D'Alessandria C., Bonanno E., Vexler V., Massari R., Trotta C., Scopinaro F., Dierckx R., Signore A. (2009). Radiolabeled humanized anti-CD3 monoclonal antibody visilizumab for imaging human T-lymphocytes. J Nucl Med.
3 Portoles P., Rojo J.M. (2009). The TCR/CD3 complex: opening the gate to successful vaccination. Curr Pharm Des.
4 Ilan, Y., E. Zigmond, G. Lalazar, A. Dembinsky, A. Ben Ya'acov, N. Hemed, I. Kasis, E. Axelrod, L. Zolotarov, A. Klein, M. El Haj, R. Gandhi, C. Baecher-Allan, H. Wu, G. Murugaiyan, P. Kivisakk, M.F. Farez, F.J. Quintana, S.J. Khoury, and H.L. Weiner, Oral Administration of OKT3 Monoclonal Antibody to Human Subjects Induces a Dose-Dependent Immunologic Effect in T Cells and Dendritic Cells. J Clin Immunol, 2009
5 Kung P., Goldstein G., Reinherz E.L., Schlossman S.F. (1979). Monoclonal antibodies defining distinctive human T cell surface antigens. Science.
6 Ochi H., Abraham M., Ishikawa H., Frenkel D., Yang K., Basso A., Wu H., Chen M.L., Gandhi R., Miller A., Maron R., Weiner H.L. (2008). New immunosuppressive approaches: oral administration of CD3-specific antibody to treat autoimmunity. J Neurol Sci.
7 Baumgart D.C., Lowder J.N., Targan S.R., Sandborn W.J., Frankel M.B. (2009). Transient cytokine-induced liver injury following administration of the humanized anti-CD3 antibody visilizumab (HuM291) in Crohn's disease. Am J Gastroenterol.
8 Baumgart, D.C., S.R. Targan, A.U. Dignass, L. Mayer, G.V. Assche, D.W. Hommes, S.B. Hanauer, U. Mahadevan, W. Reinisch, S.E. Plevy, B.A. Salzberg, A.L. Buchman, G.M. Mechkov, Z.A. Krastev, J.N. Lowder, M.B. Frankel, and W.J. Sandborn, Prospective randomized open-label multicenter phase I/II dose escalation trial of visilizumab (HuM291) in severe steroid-refractory ulcerative colitis. Inflamm Bowel Dis, 2009
9 Wing M. (2008). Monoclonal antibody first dose cytokine release syndromes-mechanisms and prediction. J Immunotoxicol.
10 Breslin S. (2007). Cytokine-release syndrome: overview and nursing implications. Clin J Oncol Nurs.
11 Cole M.S., Stellrecht K.E., Shi J.D., Homola M., Hsu D.H., Anasetti C., Vasquez M., Tso J.Y. (1999). HuM291, a humanized anti-CD3 antibody, is immunosuppressive to T cells while exhibiting reduced mitogenicity in vitro. Transplantation.
12 Carpenter P.A., Appelbaum F.R., Corey L., Deeg H.J., Doney K., Gooley T., Krueger J., Martin P., Pavlovic S., Sanders J., Slattery J., Levitt D., Storb R., Woolfrey A., Anasetti C. (2002). A humanized non-FcR-binding anti-CD3 antibody, visilizumab, for treatment of steroid-refractory acute graft-versus-host disease. Blood.
13 Kaufman A., Herold K.C. (2009). Anti-CD3 mAbs for treatment of type 1 diabetes. Diabetes Metab Res Rev.